# ^64^Cu-1,4,8,11-Tetraazacyclotetradecane-regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_

Chemical name: | ^64^Cu-1,4,8,11-Tetraazacyclotetradecane-regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_
Abbreviated name: | ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (IC_50_, 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Hydrazinonicotinic acid (HYNIC) is a coupling agent for ^99m^Tc labeling of peptides that can achieve high specific activities without affecting receptor-binding ability of the amino acid sequence. ^99m^Tc is bound to the hydrazine group, and other coordination sites could be occupied by one or more coligands. Liu et al. (13) reported the success of radiolabeling cylco(Arg-Gly-Asp-D-Phe-Lys) (c(RGDfK)) tetramer linked by glutamic acid that was conjugated with HYNIC, which showed high tumor accumulation in nude mice bearing human tumor xenografts. Boturyn et al. (14) generated a versatile molecular “Regioselectively Addressable Functionalized Template” (RAFT) platform with a cyclic decapeptide [c(-Lys(Boc)-Lys(Alloc)-Lys(Boc)-Pro-Gly-Lys(Boc)-Lys(Alloc)-Lys(Boc)-Pro-Gly-)] with two attachment sides. The upper side is linked to four copies of the c(RGDfK) peptide for targeting of integrin α_v_β_3_, and the bottom side is linked to ^99m^Tc (15) or ^111^In (16) for single-photon emission computed tomography imaging or to other labels for other imaging modalities. ^99m^Tc-RAFT-c(-RGDfK-)_4_ and ^111^In-RAFT-c(-RGDfK-)_4_ efficiently accumulated in tumors in mice. Jin et al. (17) conjugated RAFT-c(-RGDfK-)_4_ with a bifunctional chelator, 1,4,8,11-tetraazacyclotetradecane (cyclam), for radiolabeling with ^64^Cu. ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_ is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) imaging of tumor vasculature and tumor angiogenesis.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D), integrin (http://www.ncbi.nlm.nih.gov/books?term=integrin%20AND%20micad%5Bbook%5D%20AND%20table%5Btype%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+synthesis)]

Cyclam-RAFT-c(-RGDfK-)_4_ was prepared with solid-phase and solution-phase syntheses (17). Radiolabeling of cyclam-RAFT-c(-RGDfK-)_4_ was performed by heating ^64^CuCl_2_ (0.74 GBq/ml, 20 mCi/ml) and RAFT-c(-RGDfK-)_4_ (1 mM) in a 1:1 (volume:volume) ratio for 60 min at 37°C. ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_ had a radiochemical purity of >99% with a labeling efficiency of >99%. ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_ exhibited a specific activity of ~0.74 MBq/nmol (0.02 mCi/nmol) ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_ was 93% intact in mouse serum after incubation for 60 min at 37°C with little binding to serum proteins.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RAFT+RGD+AND%20in%20vitro)]

Jin et al. (17) performed in vitro assays using the human embryonic kidney (HEK) cell line stably transfected with human integrin β_1_ or β_3_ and the human glioblastoma U87MG cell line expressing β_3_. Flow cytometry analysis showed that HEK(β_3_), U87MG, and HEK(β_1_) cells exhibited high, medium, and low levels of α_v_β_3_, respectively. A cell-binding assay (n = 3) was performed using 5 nM ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_ for 1 h at 4°C. The relative binding for HEK(β_1_), HEK(β_3_), and U87MG cells were 1.8%, 6.1%, and 1.0% incubation dose/100 ug protein, respectively. Another cell-binding study (n = 6) was performed using 10 nM ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_ for 1 h at 37°C. The relative accumulation of radioactivity for HEK(β_1_), HEK(β_3_), and U87MG cells were 0.3%, 15.7%, and 0.6% incubation dose/100 ug protein, respectively. Competitive inhibition assay was performed using HEK(β_3_) and ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_. Cyclam-RAFT-c(-RGDfK-)_4_ and c(RGDfV) showed a dose-dependent inhibition of ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_ binding to HEK(β_3_), with 50% inhibition concentration values of 38.9 ± 1.4 and 2,642 ± 221 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+rodentia)]

Jin et al. (17) performed biodistribution studies of ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_ (1.0 nmol) in mice (n =5–6/group) bearing HEK(β_1_), HEK(β_3_), or U87MG tumors at 3 h after injection. ^64^Cu-Cyclam-RAFT-c(-RGDfK-)_4_ uptake was significantly higher in HEK(β_3_) (9.4 ± 1.2% injected dose/gram (ID/g)) than in U87MG (3.5 ± 0.5% ID/g) and HEK(β_1_) (1.2 ± 0.3% ID/g) at 3 h after injection (P < 0.05 between any two of the three tumor models). Prominent accumulation was observed in the kidney (20%–25% ID/g) and liver (3%–4% ID/g). The other examined normal tissues exhibited low or negligible radioactivity accumulation. The HEK(β_3_) tumor/blood and tumor/muscle ratios were ~165 and ~19, respectively. Co-injection of excess cyclam-RAFT-c(-RGDfK-)4 (150 nmol) in mice (n = 3) bearing HEK(β_3_) tumors showed >85% reduction of radioactivity in the tumors. Some inhibition was also observed in all normal tissues examined except the kidney. Autoradiography studies indicated that there is a linear correlation between the α_v_β_3_ expression and the tumor radioactivity accumulation of ^64^Cu-cyclam-RAFT-c(-RGDfK-)_4_ (R = 0.967).

PET imaging scans were performed at 1, 3, 6, and 20 h after injection in tumor-bearing mice. HEK(β_3_) and U87MG tumors were clearly visualized at all the time points in comparison to HEK(β_1_) tumors (17). The highest tumor contrast was observed at 1 h after injection for the three tumors; this was followed by a gradual washout with time. The kidneys, urinary bladder, and liver showed high radioactivity at the early time points. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Liu S., Hsieh W.Y., Jiang Y., Kim Y.S., Sreerama S.G., Chen X., Jia B., Wang F. (2007). Evaluation of a (99m)Tc-labeled cyclic RGD tetramer for noninvasive imaging integrin alpha(v)beta3-positive breast cancer. Bioconjug Chem.
14 Boturyn D., Coll J.L., Garanger E., Favrot M.C., Dumy P. (2004). Template assembled cyclopeptides as multimeric system for integrin targeting and endocytosis. J Am Chem Soc.
15 Sancey L., Ardisson V., Riou L.M., Ahmadi M., Marti-Batlle D., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2007). In vivo imaging of tumour angiogenesis in mice with the alpha(v)beta (3) integrin-targeted tracer (99m)Tc-RAFT-RGD. Eur J Nucl Med Mol Imaging.
16 Ahmadi M., Sancey L., Briat A., Riou L., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2008). Chemical and biological evaluations of an (111)in-labeled RGD-peptide targeting integrin alpha(V) beta(3) in a preclinical tumor model. Cancer Biother Radiopharm.
17 Jin Z.H., Furukawa T., Galibert M., Boturyn D., Coll J.L., Fukumura T., Saga T., Dumy P., Fujibayashi Y. (2011). Noninvasive visualization and quantification of tumor alphaVbeta3 integrin expression using a novel positron emission tomography probe, 64Cu-cyclam-RAFT-c(-RGDfK-)4. Nucl Med Biol.